# ^64^Cu-1,4,7,10-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_

Chemical name: | ^64^Cu-1,4,7,10-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_
Abbreviated name: | ^64^Cu-CBTE2A-ReCCMSH(Arg^11^)
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor, MC1R
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH)]

Malignant melanoma is the most deadly form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, pro-opiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily. However, thesereceptors have been found to be overexpressed in melanoma cells (4, 5). α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via the MC1R.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (4, 5, 7, 9, 10). 1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) has been successfully coupled to the α-MSH peptide analogs for radiolabeling with a variety of radionuclides (7). To improve the tumor/kidney uptake ratio and metabolic stability, a rhenium-cyclized α-MSH analog, Re-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ (Re-CCMSH(Arg^11^)), was conjugated with bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane (CBTE2A). CBTE2A-Re-CCMSH(Arg^11^) was radiolabeled with ^64^Cu as a potential molecular imaging agent to target melanoma (11). ^64^Cu is a positron emitter with a physical half-life of 12.7 h and is suitable for PET imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+and+synthesis)]

Wei et al. (11) reported the synthesis of ^64^Cu-CBTE2A-ReCCMSH(Arg^11^).The CBTE2A-CCMSH(Arg^11^) peptide was synthesized using standard Fmoc/HBTU(2-[1H-benzotriazole-1-yl]-l,1,3,3,-tetramethyluronium hexafluorophosphate) chemistry on an amide resin with a peptide synthesizer as reported previously by Chen et al. (10). A mixture of CBTE2A-CCMSH(Arg^11^) and trichlorooxobis-(triphenylphosphine)-rhenium (1:1 molar ratio) was incubated for 3 h at 25°C. The cyclized peptide, CBTE2A-ReCCMSH(Arg^11^), was purified with high-performance liquid chromatography (HPLC). For ^64^Cu labeling, ^64^CuCl_3_ in 0.1 M ammonium acetate was added to CBTE2A-ReCCMSH(Arg^11^) in 0.1 M ammonium acetate, and the mixture was heated for 60 min at 95ºC. Radiochemical purity (as confirmed with HPLC) was >98% with specific activities of 22–185 GBq/µmol (0.6–5 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+AND+in+vitro)]

Wei et al. (11) conducted in vitro competitive receptor-binding studies of Cu-CBTE2A-ReCCMSH and Cu-DOTA-ReCCMSH with B16/F1 murine melanoma cells that express the MC1R. The radioactive ligand was ^125^I-Tyr^2^-[Nle^4^,D-Phe^7^]α-MSH. The inhibition concentrations (IC_50_) were 5.4 nM and 6.9 nM for Cu-CBTE2A-ReCCMSH and Cu-DOTA-ReCCMSH, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+rodentia)]

Wei et al. (11) performed biodistribution studies in female C57BL/6 mice (n = 5/group) bearing 10-day-old B16/F1 murine melanoma tumors. Each mouse received 0.2 MBq (0.005 mCi (~0.01 nmol)) ^64^Cu-CBTE2A-ReCCMSH(Arg^11^). The radioactivity levels in percent injected dose per gram (% ID/g) were obtained at 30 min, 2 h, 4 h, and 24 h after injection, with tumor uptake values of 8.45 ± 1.42, 7.09 ± 3.20, 7.37 ± 1.26, and 4.01 ± 0.77, respectively. Tumor retention is high. Pre-administration of 10 nmol CBTE2A-ReCCMSH(Arg^11^) significantly reduced the tumor uptake to 0.99 ± 0.15% ID/g (P < 0.005) at 2 h after injection. No other tissues showed significant inhibition by CBTE2A-ReCCMSH(Arg^11^). The nontarget tissue uptake of ^64^Cu-CBTE2A-ReCCMSH(Arg^11^) was high at 30 min. However, the radioactivity was quickly cleared from all tissues at 2 h after injection (except kidney: 12.71 ± 1.50% ID/g at 30 min and 8.57 ± 2.51% ID/g at 2 h; e.g.,lung: 3.29 ± 1.16% ID/g at 30 min and 0.53 ± 0.06% ID/g at 2 h; blood: 2.95 ± 1.11% ID/g at 30 min and 0.19 ± 0.04% ID/g at 2 h; liver: 2.37 ± 0.28% ID/g at 30 min and 1.57 ± 0.42% ID/g at 2 h]. The fast clearance from normal tissues and high tumor retention resulted in good tumor/nontarget tissue ratios at 2 h (e.g., tumor/muscle ratio of 44). When 15 mg D-lysine was coinjected with ^64^Cu-CBTE2A-ReCCMSH(Arg^11^), the kidney and tumor radioactivity levels were decreased by >60% at 2 h after injection. In contrast, the radioactivity levels in other major tissues were not affected. PET imaging of mice bearing the B16/F1 melanomas in the neck was conducted with intravenous injection of 5.55 MBq (0.15 mCi (0.25 nmol)) ^64^Cu-CBTE2A-ReCCMSH(Arg^11^) at 0.5, 2, 4, and 24 h. At 0.5 h, the tumor, kidney, blood, lung, and heart were visible. As the background radioactivity decreased, only the tumor, kidney, liver, and bladder were clearly visible by 2 h. Pre-injection of 10 nmol CBTE2A-ReCCMSH(Arg^11^) inhibited the tumor accumulation of radioactivity by ~80% at all time points, whereas there was little effect on the kidney and liver radioactivity levels.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+AND+human)]

No publication is currently available.

## NIH Support

R24 CA86307, P50 CA103130, R24 CA86060, P30 CA91842

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
5 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Wei L., Butcher C., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Lewis J.S. (2007). Synthesis and biologic evaluation of 64Cu-labeled rhenium-cyclized alpha-MSH peptide analog using a cross-bridged cyclam chelator. J Nucl Med.